# Z_HER2:342_ Affibody-polyethylene glycol-superparamagnetic iron oxide nanoparticles

Chemical name: | Z_HER2:342_ Affibody-polyethylene glycol-superparamagnetic iron oxide nanoparticles
Abbreviated name: | IO-PEG-Z_HER2:342_
Synonym:
Agent category: | Antibody
Target: | Epidermal growth factor receptor (HER2)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=2064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes)]

Epidermal growth factor (EGF) is a 53-amino-acid growth factor (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF, with at least seven other growth factors and their transmembrane receptor kinases, play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells, such as breast, non-small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on a 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (17). These Affibody molecules exhibit high binding affinity to HER2, with K_d_ values of <50 pM. Various radiolabeled HER2 Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The synthetic Affibody molecule Cys-Z_HER2:342_ Affibody was targeted to HER2 and conjugated to superparamagnetic iron oxide coated with polyethylene glycol (IO-PEG) to form IO-PEG-Z_HER2:342_ nanoparticles (18). IO-PEG-Z_HER2:342_ nanoparticles were evaluated for magnetic resonance imaging (MRI) in nude mice bearing human SKOV3 ovarian carcinoma tumor.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20synthesis)]

IO nanoparticles (15 nm in diameter) were coated with PEG phosphatidylethanolamine (DSPE-PEG2000 amine) by hydrophobic-hydrophobic interactions (18). IO nanoparticles (10 nmol) and DSPE-PEG2000 amine (10 µmol) in chloroform (0.2 mL) were mixed, and the solvent was completely evaporated in a fume hood at room temperature. The residue was re-dissolved in water and sonicated. IO-PEG nanoparticles (27 nm in diameter) were purified with ultra-centrifugation. For conjugation with Affibody, IO-PEG (1 nmol) was first activated with the biofunctional linker 4-maleimidobutyric acid N-succinimidyl ester (1 µmol) in borate buffer (pH 8.5) for 2 h at room temperature. After column purification, Cys-Z_HER2:342_ (100 nmol) was incubated with the activated IO-PEG nanoparticles for 20 min at room temperature with a conjugation efficiency of 40%–50%. IO-PEG-Z_HER2:342_ nanoparticles were purified with column chromatography. There were ~20 Affibody molecules per nanoparticle, with a hydrodynamic diameter of 28 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20in%20vitro)]

Lee et al. (19) performed binding experiments with Cys-Z_HER2:342_ using a Biacore sensor chip immobilized with extracellular domain of chimeric HER2/Fc fusion protein. The dissociation constants (K_d_) of Z_HER2:342_ were calculated to be 30 pM for chimeric HER2/Fc fusion protein.

Gao et al. (18) determined the relaxivity (r_2_) values (7 T) of IO-PEG and Feridex (dextran-coated IO) to be 172.34 and 152.86 mM−^1^s−^1^, respectively. Cellular accumulation of IO-PEG-Z_HER2:342_ and IO-PEG nanoparticles (200, 400, and 800 µM) was determined in HER2-expressing SKOV3 cells (1 × 10^6^ cells in 5 mL medium) after 30 min of incubation. There was a dose-dependent increase in the relaxation (R_2_) with cells incubated with IO-PEG-Z_HER2:342_ nanoparticles, whereas the R_2_ values of cells incubated with IO-PEG nanoparticles remained close to those of cells incubated with medium alone. The Fe contents of cells incubated with IO-PEG-Z_HER2:342_ nanoparticles were 68 ± 22, 130 ± 20, and 270 ± 30 nmol at 200, 400, and 800 µM, respectively. On the other hand, the Fe contents of cells incubated with IO-PEG nanoparticles were 2.6, 3.4, and 9.8 nmol at 200, 400, and 800 µM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20rodentia)]

Gao et al. (18) performed in vivo T2* MRI (7 T) studies of IO-PEG-Z_HER2:342_ nanoparticles (8 nmol Fe/kg) in mice (the number of mice was not reported) bearing SKOV3 tumor at 0, 30, 60, and 90 min after intravenous injection. Only a slight decrease of MRI signal in the tumor was observed and may have been caused by an insufficient accumulation of nanoparticles (low sensitivity of MRI) in the targeted tumor. The investigators indicated that further studies are ongoing.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20human)]

No publication is currently available.

## NIH support

R21 CA121842, U54 CA119367

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
19 Lee S.B., Hassan M., Fisher R., Chertov O., Chernomordik V., Kramer-Marek G., Gandjbakhche A., Capala J. (2008). Affibody molecules for in vivo characterization of HER2-positive tumors by near-infrared imaging. Clin Cancer Res.